# Quantum dot 800–prostate-specific membrane antigen antibody J591

Chemical name: | Quantum dot 800–prostate-specific membrane antigen antibody J591
Abbreviated name: | QD800-J591
Synonym:
Agent category: | Antibody
Target: | Prostate-specific membrane antigen (PSMA), folate hydrolase
Target category: | Antigen
Method of detection: | Optical, near-infrared fluorescence (NIR) imaging
Source of signal: | Quantum dot (QD)
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&val=4758398), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nucleotide&val=4758397) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=full_report&list_uids=2346) for more information about PSMA.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Quantum%20dot%20and%20Prostate-specific%20membrane%20antigen)]

Optical fluorescence imaging is increasingly used to monitor biological functions of specific targets in small animals (1-3). However, the intrinsic fluorescence of biomolecules poses a problem when fluorophores that absorb visible light (350–700 nm) are used. Near-infrared (NIR) fluorescence (700–1,000 nm) detection avoids the background fluorescence interference of natural biomolecules, providing a high contrast between target and background tissues. NIR fluorophores have wider dynamic range and minimal background as a result of reduced scattering compared with visible fluorescence detection. They also have high sensitivity, resulting from low infrared background, and high extinction coefficients, which provide high quantum yields. The NIR region is also compatible with solid-state optical components, such as diode lasers and silicon detectors. NIR fluorescence imaging is becoming a noninvasive alternative to radionuclide imaging in small animals (4).

Fluorescent semiconductor quantum dots (QDs) are nanocrystals made of CdSe/CdTe/ZnS with radii of 1–10 nm (5-7). They can be tuned to emit signals in a range of wavelengths by changing their sizes and composition, thus providing broad excitation profiles and high absorption coefficients. They have narrow, symmetric emission spectra with long, excited-state lifetimes (20–50 ns) compared with those of fluorescent dyes (1–10 ns). They process good quantum yields of 40%–90% and possess high extinction coefficients. They are more photo-stable than conventional organic dyes. They can be coated and capped with hydrophilic materials for additional conjugation with biomolecules, such as peptides, antibodies, nucleic acids, and small organic compounds, which have been tested in vitro and in vivo (7-11). Although many cells have been labeled with QDs in vitro with little cytotoxicity, there are limited studies of long-term toxicity of QDs in small animals (12-20); little is known about the toxicity and the mechanisms of clearance and metabolism of QDs in humans.

Prostate-specific membrane antigen (PSMA) is a cell-surface glycoprotein with a molecular weight of ~100 kDa. It is a unique, type II, transmembrane-bound glycoprotein that is overexpressed on prostate tumor cells and in the neovasculature of most solid prostate tumors, but not in the vasculature of normal tissues (21, 22). This unique expression of PSMA makes it an important biomarker as well as a large extracellular target of imaging agents (23, 24). PSMA has also been detected in other tissues such as the kidneys, the proximal small intestine, and the salivary glands (22). PSMA was found to have N-acetyl α-linked acidic dipeptidase (NAALADase) or glutamate carboxypeptidase II activity (25). PSMA may play an important role in the progression of prostate cancer and glutamatergic neurotransmission, as well as in the absorption of folate (26). In the central nervous system, PSMA metabolizes N-acetyl-aspartyl-glutamate, and in the proximal small intestine it removes γ-linked glutamates from poly-γ-glutamate folate and folate hydrolase (22). PSMA can be used as a marker for the detection of metastatic cancers with imaging agents. Although the commercially available monoclonal antibody ^111^In-labeled Capromomab pendetide (http://www.ncbi.nlm.nih.gov/bookshelf/br.fcgi?book=micad&part=Capromab111In) (^111^In-CYT-356) is in clinical use for the detection of prostate cancer, the results obtained with this antibody are not entirely reliable (27). In addition, this antibody has limited access to tumors and may produce low signal/noise ratios because the target is the intracellular domain of PSMA (28, 29). J591, a monoclonal antibody against the extracellular domain of PSMA (30), was conjugated to QD655 (QD655-J591) and was found to accumulate in a human prostate cancer cell line in vitro and in nude mice (15). However, QD655-J591 has suboptimal tissue penetration and autofluorescence from the skin.To improve this approach, Shi et al. (31) used an anti-PSMA antibody J591conjugate with QDs (QD800-J591), which emit light in the NIR 800-nm range.

### Related Resource Links:

- Chapters in MICAD (PSMA (http://www.ncbi.nlm.nih.gov/books?term=PSMA%5BAll%20Fields%5D%20AND%20micad%5Bbook%5D))
- Gene information in NCBI (PSMA (http://www.ncbi.nlm.nih.gov/gene/2346)).
- Articles in Online Mendelian Inheritance in Man (OMIM) (PSMA (http://www.ncbi.nlm.nih.gov/omim/600934))
- Clinical trials (J591 (http://www.clinicaltrials.gov/ct2/results?term=J591))
- Drug information in FDA (J591 (http://google2.fda.gov/search?q=j591&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=9&y=8))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Quantum%20dot%20and%20Prostate-specific%20membrane%20antigen%20and%20synthesis)]

Non-cadmium–based QDs (InAs/InP/ZnSe) with polyethylene glycol (PEG) modification were activated using the hetero-bifunctional cross-linker 4-(maleimidomethyl)-1-cyclohexanecarboxylic acid N-hydroxysuccinimide ester (SMCC), yielding a maleimide-nanocrystal surface (31). PSMA monoclonal antibody J591 was reduced with dithiothreitol (DTT) to expose free sulfhydryl functional groups. Excess SMCC and DTT were removed with column chromatography. Activated QD800 PEG conjugates were mixed with the reduced J591 at a ratio of 1:3 and then covalently coupled. The resultant QD800-J591 conjugates were concentrated by ultrafiltration and purified using column chromatography. QD800-J591 emits light at the NIR fluorescence range of 800 nm. The hydrodynamic diameter of QD800-J591 and the number of J591 molecules per DQ were not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Quantum%20dot%20and%20Prostate-specific%20membrane%20antigen%20and%20in%20vitro)]

LNCaP human prostate cancer cells were reported to have a K_d_ of 1.83 nM with ^131^I-labeled J591 and a B_max_ of 600,000–800,000 sites/cell in a saturation binding assay (30). Binding studies of QD800-J591 and QD800-PEG were performed using human prostate cancer cell lines C4-2 (a subclone of LNCaP that is positive for PSMA) and PC-3 (negative for PSMA) (31). QD800-J591 was shown to bind to C4-2 cells, whereas QD800-PEG did not bind to C4-2 cells. No fluorescence was detected on the cell surface of PC-3 cells with QD800-J591. QD800-J591 bound specifically to C4-2 cells, given that PC-3 cells without PSMA showed no binding by QD800-J591. QD800-J591 showed no obvious toxicity to C4-2 cells in culture.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Quantum%20dot%20and%20Prostate-specific%20membrane%20antigen%20and%20rodentia)]

Tumor-imaging studies of QD800-J591 were performed in nude mice bearing a C4-2 tumor in the mouse tibia (31). Whole-body small animal images were obtained with reflectance planar fluorescence after intravenous injection of QD800-J591 and QD800-PEG. Intense tumor signals were obtained with QD800-J591 (0.1 nmol In) at 30 min after injection (active targeting by specific antibody–antigen recognition). The tumor/background ratio was 2.7. Little tumor fluorescence signals were obtained with QD800-PEG at 30 min after injection (passive targeting by enhanced vascular permeability of tumor). No blocking experiments (with unconjugated J591) were performed.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Quantum%20dot%20and%20Prostate-specific%20membrane%20antigen%20and%20%28dog%20or%20pig%20or%20rabbit%20or%20sheep%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Quantum%20dot%20and%20Prostate-specific%20membrane%20antigen%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Quantum%20dot%20and%20Prostate-specific%20membrane%20antigen%20and%20human%20not%20animal%20not%20cell%20line)]

No publication is currently available.

## References

1 Achilefu S. (2004). Lighting up tumors with receptor-specific optical molecular probes. Technol Cancer Res Treat.
2 Becker A., Hessenius C., Licha K., Ebert B., Sukowski U., Semmler W., Wiedenmann B., Grotzinger C. (2001). Receptor-targeted optical imaging of tumors with near-infrared fluorescent ligands. Nat Biotechnol.
3 Ntziachristos V., Bremer C., Weissleder R. (2003). Fluorescence imaging with near-infrared light: new technological advances that enable in vivo molecular imaging. Eur Radiol.
4 Tung C.H. (2004). Fluorescent peptide probes for in vivo diagnostic imaging. Biopolymers.
5 Chan W.C., Maxwell D.J., Gao X., Bailey R.E., Han M., Nie S. (2002). Luminescent quantum dots for multiplexed biological detection and imaging. Curr Opin Biotechnol.
6 Gao X., Nie S. (2005). Quantum dot-encoded beads. Methods Mol Biol.
7 Michalet X., Pinaud F.F., Bentolila L.A., Tsay J.M., Doose S., Li J.J., Sundaresan G., Wu A.M., Gambhir S.S., Weiss S. (2005). Quantum dots for live cells, in vivo imaging, and diagnostics. Science.
8 Alivisatos A.P., Gu W., Larabell C. (2005). Quantum dots as cellular probes. Annu Rev Biomed Eng.
9 Hilger I., Leistner Y., Berndt A., Fritsche C., Haas K.M., Kosmehl H., Kaiser W.A. (2004). Near-infrared fluorescence imaging of HER-2 protein over-expression in tumour cells. Eur Radiol.
10 Medintz I.L., Uyeda H.T., Goldman E.R., Mattoussi H. (2005). Quantum dot bioconjugates for imaging, labelling and sensing. Nat Mater.
11 Smith A.M., Gao X., Nie S. (2004). Quantum dot nanocrystals for in vivo molecular and cellular imaging. Photochem Photobiol.
12 Akerman M.E., Chan W.C., Laakkonen P., Bhatia S.N., Ruoslahti E. (2002). Nanocrystal targeting in vivo. Proc Natl Acad Sci U S A.
13 Braydich-Stolle L., Hussain S., Schlager J.J., Hofmann M.C. (2005). In vitro cytotoxicity of nanoparticles in mammalian germline stem cells. Toxicol Sci.
14 Frangioni J.V., Hajjar R.J. (2004). In vivo tracking of stem cells for clinical trials in cardiovascular disease. Circulation.
15 Gao X., Cui Y., Levenson R.M., Chung L.W., Nie S. (2004). In vivo cancer targeting and imaging with semiconductor quantum dots. Nat Biotechnol.
16 Han M., Gao X., Su J.Z., Nie S. (2001). Quantum-dot-tagged microbeads for multiplexed optical coding of biomolecules. Nat Biotechnol.
17 Lovric J., Bazzi H.S., Cuie Y., Fortin G.R., Winnik F.M., Maysinger D. (2005). Differences in subcellular distribution and toxicity of green and red emitting CdTe quantum dots. J Mol Med.
18 Ohnishi S., Lomnes S.J., Laurence R.G., Gogbashian A., Mariani G., Frangioni J.V. (2005). Organic alternatives to quantum dots for intraoperative near-infrared fluorescent sentinel lymph node mapping. Mol Imaging.
19 Shiohara A., Hoshino A., Hanaki K., Suzuki K., Yamamoto K. (2004). On the cyto-toxicity caused by quantum dots. Microbiol Immunol.
20 Soltesz E.G., Kim S., Laurence R.G., DeGrand A.M., Parungo C.P., Dor D.M., Cohn L.H., Bawendi M.G., Frangioni J.V., Mihaljevic T. (2005). Intraoperative sentinel lymph node mapping of the lung using near-infrared fluorescent quantum dots. Ann Thorac Surg.
21 Feneley M.R., Jan H., Granowska M., Mather S.J., Ellison D., Glass J., Coptcoat M., Kirby R.S., Ogden C., Oliver R.T., Badenoch D.F., Chinegwundoh F.I., Nargund V.H., Paris A.M., Britton K.E. (2000). Imaging with prostate-specific membrane antigen (PSMA) in prostate cancer. Prostate Cancer Prostatic Dis.
22 Ghosh A., Heston W.D. (2004). Tumor target prostate specific membrane antigen (PSMA) and its regulation in prostate cancer. J Cell Biochem.
23 Nanus, D.M., M.I. Milowsky, L. Kostakoglu, P.M. Smith-Jones, S. Vallabahajosula, S.J. Goldsmith, and N.H. Bander, Clinical use of monoclonal antibody HuJ591 therapy: targeting prostate specific membrane antigen. J Urol, 2003170(6 Pt 2): p. S84-8; discussion S88-9.
24 Nargund V., Al Hashmi D., Kumar P., Gordon S., Otitie U., Ellison D., Carroll M., Baithun S., Britton K.E. (2005). Imaging with radiolabelled monoclonal antibody (MUJ591) to prostate-specific membrane antigen in staging of clinically localized prostatic carcinoma: comparison with clinical, surgical and histological staging. BJU Int.
25 Luthi-Carter R., Barczak A.K., Speno H., Coyle J.T. (1998). Molecular characterization of human brain N-acetylated alpha-linked acidic dipeptidase (NAALADase). J Pharmacol Exp Ther.
26 O'Keefe, D., D. Bachich, and W.D. Heston, Prostate specific membrane antigen. Prostate cancer, biology, genetics, and the new therapeutics., ed. L. Chung, W. Issacs, and J. Simons. 2001, New Jersey: Humana Press. 307-326.
27 Ponsky L.E., Cherullo E.E., Starkey R., Nelson D., Neumann D., Zippe C.D. (2002). Evaluation of preoperative ProstaScint scans in the prediction of nodal disease. Prostate Cancer Prostatic Dis.
28 Sundaresan G., Yazaki P.J., Shively J.E., Finn R.D., Larson S.M., Raubitschek A.A., Williams L.E., Chatziioannou A.F., Gambhir S.S., Wu A.M. (2003). 124I-labeled engineered anti-CEA minibodies and diabodies allow high-contrast, antigen-specific small-animal PET imaging of xenografts in athymic mice. J Nucl Med.
29 Jain R.K. (1999). Transport of molecules, particles, and cells in solid tumors. Annu Rev Biomed Eng.
30 Smith-Jones P.M., Vallabahajosula S., Goldsmith S.J., Navarro V., Hunter C.J., Bastidas D., Bander N.H. (2000). In vitro characterization of radiolabeled monoclonal antibodies specific for the extracellular domain of prostate-specific membrane antigen. Cancer Res.
31 Shi C., Zhu Y., Xie Z., Qian W., Hsieh C.L., Nie S., Su Y., Zhau H.E., Chung L.W. (2009). Visualizing human prostate cancer cells in mouse skeleton using bioconjugated near-infrared fluorescent quantum dots. Urology.